# ^111^In-Labeled DTPA-conjugated Tat-linked anti-phosphorylated histone protein H2AX antibody

Chemical name: | ^111^In-Labeled DTPA-conjugated Tat-linked anti-phosphorylated histone protein H2AX antibody
Abbreviated name: | [^111^In]-DTPA-anti-γH2AX-Tat
Synonym:
Agent Category: | Antibody
Target: | Histone protein γH2AX (gamma H2AX)
Target Category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=histone%20protein%20H2AX&cmd=DetailsSearch)]

Chemotherapy and radiotherapy, or a combination of the two, are often used to treat cancer and are known to either damage cellular DNA itself or to interfere with the DNA metabolic pathways and generate DNA double-strand breaks (dsb) that are fatal for the neoplastic cells (1). Because the generation of dsb by these therapies is the main cause of cell death, the variable capacity of a cell to repair the dsb influences its survival response to these treatments. In other words, the cell will survive only if the dsb is quickly repaired; otherwise, the cell will probably die (2). Therefore, the visualization of DNA dsb in tumor cells can provide useful information regarding the efficacy of a cancer treatment regimen and can also predict the prognosis for a patient (3). The repair of DNA dsb in the cell is initiated by the phosphorylation of H2AX, a histone protein, to γH2AX, which initiates a signaling pathway to attract dsb repair proteins (such as DNA-dependent protein kinase, breast cancer type 1 susceptibility protein, etc.) at the site of DNA damage. As a consequence, compared to normal cells, the expression and phosphorylation of H2AX is elevated in the neoplastic cells that are subject to genotoxic insult, which results in the accumulation of this protein and the formation of foci at the location of DNA injury (2). Current immunohistochemical and flow cytometric methods using an anti-γH2AX antibody (Ab) are utilized to detect dsb in tumor cells before and after an anti-cancer treatment of a patient, but these procedures are invasive and time-consuming (1).

Visualization of γH2AX in the cell with non-invasive imaging techniques before and after anti-cancer treatment can be an excellent alternative to invasive procedures and can help in the rapid assessment of an intervention (4). However, the major limitations of imaging DNA dsb are that the strand breaks are located in the nucleus and are protected by the cell and the nuclear membranes. In addition to this limitation, imaging agents (including antibodies) that target γH2AX may not be able to penetrate the protective membranes and generate a signal that can be captured to visualize the dsb. Cornelissen et al. hypothesized that if the anti-γH2AX antibody was to be used as a probe to detect DNA dsb within the cellular nucleus, it will not only require assistance to penetrate the membranes but will have to be labeled with an appropriate tracer, such as a radionuclide, to visualize the dsb with imaging techniques (4). To test this hypothesis, the anti-γH2AX Ab was tagged with the Tat peptide, which contains a short HIV-1 transactivator of the transcription amino acid sequence that facilitates the transport of proteins or other molecules across the cell and nuclear membranes. The anti-γH2AX Ab-Tat complex was then labeled with ^111^In and Cy3, AF555, or AF888 (a group of fluorophores), respectively (4). In a set of proof-of-principal studies, the fluorophore-labeled Ab-Tat conjugate was then evaluated for the optical imaging of dsb under in vitro conditions (using human mouse embryonic cell lines). In addition, the fluorophore- or radionuclide-labeled Ab probes were investigated for the visualization of MDA-MB-468 cell xenograft tumors (a human breast cancer cell line) in mice, using fluorescence imaging (for animals injected with the Cy3-Ab-Tat conjugate) and single-photon emission computed tomography (SPECT; for animals injected with the [^111^In]-Ab-Tat conjugate). The biodistribution of [^111^In]-DTPA-anti-γH2AX-Tat in the tumor-bearing mice was also investigated.

### Related Resource Links

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_002096.1) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_002105.2) sequences of human histone protein HA2X

Gene (http://www.ncbi.nlm.nih.gov/nuccore?Db=gene&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_gene&IdsFromResult=52630339) of H2AX (Gene ID: 3014)

H2AX in Online Mendelian Inheritance in Man Database (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=gene&Cmd=Link&LinkName=gene_omim&LinkReadableName=OMIM&IdsFromResult=3014)

Inhibitors of H2AX in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Inhibitors%20of%20H2AX%20histone)

H2AX gene function in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H2AX%20gene%20function%20)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28111%29In-anti-%u03B3H2AX-Tat&cmd=DetailsSearch)]

The source of the polyclonal rabbit anti-γH2AX Ab and the synthesis of [^111^In]-DTPA-anti-γH2AX-Tat have been described by Cornelissen et al. (4). The radiochemical yield (RCY) of the radioimmuno-conjugate (RIC) was ≥95% as determined with instant thin-layer chromatography. Size-exclusion radio high-performance liquid chromatography revealed that the chemical and radiochemical purity (RCP) of the RIC was >95%. The specific activity (SA) of the labeled Ab was reported to be 0.5–6 MBq/μg (13.5–162 μCi/μg).

For use as a control, [^111^In]-DTPA-anti-mouse IgG-Tat ([^111^In]-DTPA-anti-mIgG-Tat) was also synthesized as detailed elsewhere (4). The RCY, RCP, and SA of the control RIC were not reported (4).

The fluorophore (Cy3, AF488, or AF555)-anti-γH2AX-Tat and the fluorophore-anti-mIgG-Tat conjugates were respectively synthesized as described, and the Cy3/IgG ratio in each complex was reported to be 6:1 (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28111In%29%20gamma%20H2AX-Tat%20in%20vitro%20studies&cmd=DetailsSearch)]

An immunofluorescence assay was used to detect the induction of γH2AX in irradiated MDA-MB-468 cells (4). The induction of γH2AX in these cells was also confirmed with Western blot analysis.

Using a whole-cell lysate of irradiated 231-H2H cells (a human breast cancer MDA-MB-231 cell line transfected with the HER2 gene) to induce γH2AX in a radioimmuno competition assay, the log of 50% inhibitory concentrations (log(IC_50_)) of DTPA-anti-γH2AX-Tat and the anti-γH2AX Ab to compete with [^111^In]-DTPA-anti-γH2AX-Tat for binding to γH2AX were determined (4). The log(IC_50_) values of the Tat-linked and the native Abs were reported to be 0.33 ± 0.12 and 0.42 ± 0.14 nmol/L, respectively (P = 0.70), indicating that the affinity of DTPA-anti-γH2AX-Tat for γH2AX was similar to that of native anti-γH2AX Ab.

Cell internalization studies with [^111^In]-DTPA-anti-γH2AX-Tat and [^111^In]-DTPA-anti-mIgG-Tat showed that the RICs had similar internalization profiles in irradiated and non-irradiated (control) MDA-MB-468 whole cells, including the nuclei (4).

The retention of [^111^In]-DTPA-anti-γH2AX-Tat and [^111^In]-DTPA-anti-mIgG-Tat was investigated in irradiated and non-irradiated MDA-MB-468 cells (4). The retention half-life of [^111^In]-DTPA-anti-γH2AX-Tat in the irradiated cells was 27.71 ± 11.01 h compared to 1.81 ± 0.87 h in the non-irradiated cells. For [^111^In]-DTPA-anti-mIgG-Tat, the retention half-life in the irradiated cells was 0.23 ± 0.09 h under the same experimental conditions. From this study, the investigators concluded that the labeled anti-γH2AX-Tat tracer was retained only by irradiated cells with induced γH2AX (4).

To visualize DNA dsb, MDA-MB-468 cells were exposed to AF488-anti-γH2AX-Tat or AF488-anti-mIgG-Tat and irradiated or sham-irradiated as described by Cornelissen et al. (4). Confocal nuclear fluorescence microscopy revealed that fluorescence due to AF488 was visible only in the irradiated cells exposed to AF488-anti-γH2AX-Tat and that the fluorescence signal was colocalized with the γH2AX foci in the cells.

To confirm that the retention of fluorophore-labeled anti-γH2AX-Tat was dependent on the presence of γH2AX, wild-type (WT) and H2AX-null mouse embryo fibroblasts were exposed to Cy3-anti-γH2AX-Tat and irradiated or sham-irradiated as before (4). Colocalization of Cy3 with the γH2AX foci was apparent only in the irradiated WT cells at 1 h after irradiation and was not visible in the cells at 23 h after irradiation. This indicated that there was a rapid repair of DNA dsb damage in the WT cells and that Cy3-anti-γH2AX-Tat accumulated specifically in the irradiated cell nuclei containing the γH2AX foci.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28111%29In-anti-%u03B3H2AX-Tat%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DTPA-anti-γH2AX-Tat was investigated in mice (n = 3 animals/group) bearing MDA-MB-468 cell xenograft tumors on the right hind limb (4). The rodents were either administered bleomycin (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15036) (10 μg; delivered through an intraperitoneal injection) or x-ray irradiated (0–10 Gy) at the tumor site 2 h and 1 h, respectively, prior to intravenous injection of the labeled Ab-Tat complex. Control animals did not receive the bleomycin or x-ray treatment. For comparison, another group of animals received an intravenous injection of [^111^In]-DTPA-anti-mIgG-Tat. The animals were euthanized at predetermined time points postinjection (p.i.), and all the major organs, including tumors, were collected to determine the amount of accumulated radioactivity. The uptake data were reported as percent of injected dose per gram tissue (% ID/g). At each time point, the uptake of label was higher in tumors of mice injected the anti-γH2AX-Tat Ab compared with tumors obtained from animals injected with the IgG-Tat tracer. At 24 hours p.i., the uptake of label in the tumor was 3.6 ± 0.1% ID/g with [^111^In]-DTPA-anti-γH2AX-Tat compared to 1.2 ± 0.1% ID/g with [^111^In]-DTPA-mIgG-Tat (P < 0.0001). In addition, the uptake of radioactivity from [^111^In]-DTPA-anti-mIgG-Tat in tumors of mice treated with bleomycin or x-rays remained relatively constant at this time point (1.7 ± 0.7% ID/g and 1.7 ± 0.2% ID/g, respectively) compared to tumors of the untreated control mice (1.2 ± 0.1% ID/g; P > 0.05). At 24 p.i., the amount of radioactivity from radiolabeled anti-γH2AX-Tat in tumors of mice treated with bleomycin and x-rays was 5.4 ± 1.2% ID/g and 5.2 ± 0.6% ID/g, respectively, which was significantly higher (P < 0.0001) than the accumulation in tumors of the untreated controls (3.6 ± 0.1% ID/g). At 72 h p.i., the amount of radioactivity in tumors of mice treated with bleomycin remained high (6.68 ± 0.71% ID/g), but the label was reduced to baseline levels (2.56 ± 0.36% ID/g) in tumors of the irradiated animals. Little difference in the accumulation of radioactivity (both with [^111^In]-DTPA-anti-γH2AX-Tat and [^111^In]-DTPA-anti-mIgG-Tat) was observed in normal tissues of the non-irradiated, bleomycin-treated, or irradiated animals (4).

In another study, the correlation between the induction of γH2AX in the tumor due to irradiation and the uptake of label from [^111^In]-DTPA-anti-γH2AX-Tat was investigated (4). For this, mice were injected with [^111^In]-DTPA-anti-γH2AX-Tat and exposed to increasing doses of x-rays. SPECT images were acquired from the animals at 23 h p.i., and a positive correlation between the accumulation of ^111^In in the tumor and the x-ray dose was evident (Spearman r = 0.9; P = 0.042). Histological staining of tumor sections confirmed that expression of γH2AX in the tumor cells increased with the dose of irradiation.

Groups of mice bearing MDA-MB-468 cell xenograft tumors were also administered Cy3-mIgG-Tat or Cy3-anti-γH2AX-Tat and irradiated as described above to induce γH2AX in the lesions (4). Fluorescent images of the animals were acquired at various time points, and Cy3 was observed to accumulate only in the irradiated tumors of mice injected with Cy3-anti-γH2AX-Tat. The fluorescent signal peaked in the irradiated tumors at 48 h p.i. and decreased to baseline levels at 72 h p.i. No fluorescence was detected in tumors of control animals or in tumors of mice injected with Cy3-anti-mIgG-Tat.

From these studies, the investigators concluded that anti-γH2AX-Tat immunoconjugates can be used with imaging techniques to detect DNA dsb in rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28111%29In-anti-%u03B3H2AX-Tat%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28111%29In-anti-%u03B3H2AX-Tat%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=(111)In-anti-%CE%B3H2AX-Tat%20Human%20Studies)]

No publication is currently available.

.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Redon C.E., Nakamura A.J., Zhang Y.W., Ji J.J., Bonner W.M., Kinders R.J., Parchment R.E., Doroshow J.H., Pommier Y. (2010). Histone gammaH2AX and poly(ADP-ribose) as clinical pharmacodynamic biomarkers. Clin Cancer Res.
2 Sak A., Stuschke M. (2010). Use of gammaH2AX and other biomarkers of double-strand breaks during radiotherapy. Semin Radiat Oncol.
3 Dickey J.S., Redon C.E., Nakamura A.J., Baird B.J., Sedelnikova O.A., Bonner W.M. (2009). H2AX: functional roles and potential applications. Chromosoma.
4 Cornelissen B., Kersemans V., Darbar S., Thompson J., Shah K., Sleeth K., Hill M.A., Vallis K.A. (2011). Imaging DNA Damage In Vivo Using {gamma}H2AX-Targeted Immunoconjugates. Cancer Res.